# 6-Iodo-2-[4'-N-(2-[^18^F]fluoroethyl)methylamino]phenylimidazo[1,2-a]pyridine

Chemical name: | 6-Iodo-2-[4'-N-(2-[^18^F]fluoroethyl)methylamino]phenylimidazo[1,2-a]pyridine
Abbreviated name: | [^18^F]FEM-IMPY
Synonym:
Agent Category: | Compound
Target: | Aggregates of ß-amyloid (Aß) peptides
Target Category: | Acceptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%226-iodo-2-%284%27-N-%282-fluoroethyl%29methylamino%29phenylimidazo%281%2C2-a%29pyridine%22%5BSubstance%20Name%5D%20OR%20FEM-IMPY%5BText%20Word%5D)]

Alzheimer’s disease (AD) is a major neurodegenerative disease associated with an irreversible decline of mental functions and with cognitive impairment (1). It is characterized by the presence in the brain of senile plaques of β-amyloid (Aβ) peptides with intracellular neurofibrillary tangles of filaments that contain the hyperphosphorylated protein tau (2, 3). Accelerated deposition of Aβ deposits seems to be a key risk factor associated with AD, and although the mechanisms of the disease are still not fully understood, reducing the deposition of amyloid plaques seems to benefit patients.

Several radioligands for positron emission tomography (PET) have been developed (4-6) and tested in humans as in vivo diagnostic tools for imaging and measuring the formation of Aβ deposits (6). The first agent successfully used in human studies was [^18^F]FDDNP (7), a malonitrile derivative found to bind to both neurofibrillary tangles and Aβ plaques. The second successful attempt was made with [^11^C]PIB (8), also known as Pittsburgh Compound B or [^11^C]6-OH-BTA-1, which showed marked retention in areas of the cortex known to contain substantial amounts of Aβ deposits. The third PET radioligand successfully tested in humans was [^11^C]4-N-methylamino-4´-hydroxystilbene, a stilbene derivative commonly named [^11^C]SB-13 that exhibited good binding affinities for Aβ aggregates in vitro, moderate lipophilicity, high initial brain uptake in the normal rat cortex, and a rapid washout (9).

Benzofuran derivatives labeled with radioactive iodine have shown very good binding affinities for Aβ aggregates and good brain penetration (10). Unfortunately, their level of nonspecific binding was found to be very high, which makes them unsuitable for in vivo plaque imaging. However, [^125^I]IMPY displayed a good initial brain uptake and rapid washout from normal mouse brain and postmortem AD brain sections (11). Its desirable pharmacokinetics makes [^125^I]IMPY an attractive agent for mapping Aβ plaques. More recently, the ^18^F-labeled analog of IMPY in which the N-methyl group is replaced with [^18^F]2-fluoroethyl ([^18^F]FEM-IMPY) has been synthesized and is currently under investigation as a prospective PET radioligand for Aβ plaques (12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEM-IMPY%20AND%20synthesis%5BAll%20Fields%5D)]

A one-pot radiosynthesis of [^18^F]FEM-IMPY using HM-IMPY as the precursor was developed by Cai et al. (12). In this method, HM-IMPY reacted with ethyleneglycol bis-tosylate at 130–150°C under microwave conditions. This slow reaction (5% complete after 10 min) could be enhanced by the addition of [K-(Kryptofix 222)]^+^[F]^–^, which accelerated the alkylation to generate FEM-IMPY with a 70–80% yield under anhydrous conditions. At the end of the synthesis, the radiochemical purity of the radiotracer was >93% and its specific radioactivity was 85–662 GBq/µmol (2.3–17.9 Ci/µmol).

The synthesis of the precursor HM-IMPY could be achieved in one step under mild conditions by bromination of the secondary amine 4-methylaminocetaphenone using tetra-n-butylammonium tribromide in MeOH (13). This bromination was regioselective (only on the methyl group) and did not produce any byproducts on the ring from bromination.

An alternative synthesis of HM-IMPY is to follow one of the methods reported in the literature for the demethylation of N,N-dimethylanilines to perform a monodemethylation of the imidazopyridine IMPY (14). One of the approaches used TiCl_4_/CH_2_Cl_2_ and only produced polymerized compounds (15). In the other approach, tetra-n-butylammonium periodate, a potent oxygen donor, was used to hydroxylate one of the methyl groups in the presence of a metalloporphyrin catalyst. Those two methods were not very successful: the first produced polymerized products only and the second led to low yields with many side reactions and had to be abandoned.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEM-IMPY%20AND%20in%20vitro)]

FEM-IMPY was found to compete well with [^125^I]TZDM, a probe selective for Aβ plaques previously reported in the literature (16). Studies of binding to Aβ-40 aggregates in solution and AD brain homogenates led to an inhibition constant (K_i_) of 27 ± 8 nM. The high lipophilicity (Log D value of 4.41 ± 0.10 at pH 7.4) of FEM-IMPY might explain the relatively high nonspecific binding of [^18^F]FEM-IMPY to human AD brain homogenates (~50% of the total binding) (12).

Incubation of mouse brain homogenates with [^18^F]FEM-IMPY at 37°C for various lengths of time resulted in radioactive polar and lipophilic metabolites and parent [^18^F]FEM-IMPY (12). A mass spectrum analysis of the metabolites showed the presence of a dealkylated aromatic amino group, consistent with the fact that tertiary amino groups are unstable in an oxidative environment. Complete N-dealkylation of [^18^F]FEM-IMPY was not observed in vitro; the metabolism ended after the radioligand was degraded to ~10% conversion.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEM-IMPY%20AND%20rodentia%5BMeSH%5D)]

Cai et al. (12) performed in vivo biodistribution studies on 4 normal male ICR mice (2–3 months-old) injected intravenously with a saline solution of [^18^F]FEM-IMPY [14.8–16.5 MBq (0.4–0.5 mCi)]. Results showed that the radiotracer easily penetrated the blood–brain barrier, and a peak of the brain uptake [~6.4% injected dose/g (% ID/g)] was observed at 0.5 min after injection. This value compared well with [^123,125^I]IMPY (7.2% ID/g in 2 min). However, the washout of radioactivity for [^18^F]FEM-IMPY in normal mice was found to be biphasic (rapid over the first 20 min and much slower thereafter), whereas a single-exponential washout was observed for [^123,125^I]IMPY. Residual brain radioactivity was 4.5% ID/g for [^18^F]FEM-IMPY at 2 h after injection.

A high-performance liquid chromatography analysis of homogenates of ex vivo mouse brain after injection of the radioligand showed that the residual activity represented polar metabolites (presumably a fluoride ion or a related small-molecule ionic species such as [^18^F]FCH_2_CO_2_^–^) and was not the result of nonspecific binding. Lipophilicity of the ligands did not seem to play a role, and the contribution of the lipophilic intermediate was unclear at the time of the study. Given its low concentration observed both in vivo and in vitro, it might not have contributed significantly to the TACs.

Substantial bone uptake of [^18^F]FEM-IMPY was observed in the skull. Substitution of the 4-ethylene protons by deuterium led to a 34% reduction of the radioactivity in the skull, while there was no effect on brain uptake or clearance of the radiotracer.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEM-IMPY%20AND%20%28dog%20OR%20sheep%20OR%20pig%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEM-IMPY%20AND%20%28%28primate%20NOT%20human%29%20OR%20baboon%20OR%20monkey%29)]

Cai et al. (12) performed brain PET scans on a male rhesus monkey (7.12 kg) after intravenous administration of 107.3 MBq (2.9 mCi) of [^18^F]FEM-IMPY. The experiment involved acquiring dynamic transaxial images over a period of 120 min with scan duration ranging from 30 s to 5 min.

Results showed a rapid increase of brain activity, with peak values of 0.26–0.35% ID/g at 3–6 min after injection. [^18^F]FEM-IMPY appeared to be washed out of all brain regions in a similar fashion, with a monoexponential washout rate of 0.05–0.09 min^-1^ (0.0488 ± 0.0020 min^-1^ for the brain stem, 0.0606 ± 0.0024 min^-1^ for the frontal cortex, 0.0859 ± 0.0037 min^-1^ for the striatum, and 0.0488 ± 0.0020 min^-1^ for the cerebellum), which corresponds to a half-life (t_1/2_) of 8–14 min. Activity in bone increased exponentially and reached levels of ~0.1% ID kg/g, which is similar to residual activity in the brain and substantially less than what was observed in mice. The studies by Cai et al. (12) showed that the metabolism of [^18^F]FEM-IMPY was significantly slower in rhesus monkeys than in mice.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEM-IMPY%20AND%20human)]

No publication is currently available.

## References

1 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
3 Brandt R., Leschik J. (2004). Functional interactions of tau and their relevance for Alzheimer's disease. Curr Alzheimer Res.
4 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
5 Bacskai B.J., Hickey G.A., Skoch J., Kajdasz S.T., Wang Y., Huang G.F., Mathis C.A., Klunk W.E., Hyman B.T. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
6 Wu C., Pike V.W., Wang Y. (2005). Amyloid imaging: from benchtop to bedside. Curr Top Dev Biol.
7 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
8 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
9 Ono M., Wilson A., Nobrega J., Westaway D., Verhoeff P., Zhuang Z.P., Kung M.P., Kung H.F. (2003). 11C-labeled stilbene derivatives as Abeta-aggregate-specific PET imaging agents for Alzheimer's disease. Nucl Med Biol.
10 Ono M., Kung M.P., Hou C., Kung H.F. (2002). Benzofuran derivatives as Abeta-aggregate-specific imaging agents for Alzheimer's disease. Nucl Med Biol.
11 Kung M.P., Hou C., Zhuang Z.P., Zhang B., Skovronsky D., Trojanowski J.Q., Lee V.M., Kung H.F. (2002). IMPY: an improved thioflavin-T derivative for in vivo labeling of beta-amyloid plaques. Brain Res.
12 Cai L., Chin F.T., Pike V.W., Toyama H., Liow J.S., Zoghbi S.S., Modell K., Briard E., Shetty H.U., Sinclair K., Donohue S., Tipre D., Kung M.P., Dagostin C., Widdowson D.A., Green M., Gao W., Herman M.M., Ichise M., Innis R.B. (2004). Synthesis and evaluation of two 18F-labeled 6-iodo-2-(4'-N,N-dimethylamino)phenylimidazo[1,2-a]pyridine derivatives as prospective radioligands for beta-amyloid in Alzheimer's disease. J Med Chem.
13 Kajigaeshi S., Kakinami T., Okamoto T., Fujisaki S. (1987). Synthesis of bromoacetyl derivatives by use of tetrabutylammonium tribromide. Bull. Chem. Soc. Jpn.
14 Zhuang Z.P., Kung M.P., Wilson A., Lee C.W., Plossl K., Hou C., Holtzman D.M., Kung H.F. (2003). Structure-activity relationship of imidazo[1,2-a]pyridines as ligands for detecting beta-amyloid plaques in the brain. J Med Chem.
15 Periasamy M., Jayakumar K.N., Bharathi P. (2000). Aryltitanium species through the reaction of N,N-dialkylarylamines with TiCl(4): oxidative coupling, N-dealkylation, and reaction with electrophiles. J Org Chem.
16 Zhuang Z.P., Kung M.P., Hou C., Skovronsky D.M., Gur T.L., Plossl K., Trojanowski J.Q., Lee V.M., Kung H.F. (2001). Radioiodinated styrylbenzenes and thioflavins as probes for amyloid aggregates. J Med Chem.